# Transferrin-coated gadolinium-labeled human serum albumin nanoparticles

Chemical name: | Transferrin-coated gadolinium-labeled human serum albumin nanoparticles
Abbreviated name: | Gd-HSA-Tf-NP
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Gd
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Nanoparticles&cmd=DetailsSearch)]

It is necessary to use small molecule contrast agents (CAs) to generate a good contrast in images produced with magnetic resonance imaging (MRI) for the proper diagnosis and monitoring of diseases. Small molecule CAs improve the contrast of only the intravascular tissues, do not cross biological barriers such as the blood–brain barrier (BBB), and are rapidly cleared from circulation through the kidneys (1). Therefore, these CAs cannot be used with MRI for the noninvasive imaging of the brain. As a result, there is an urgent need to develop CAs that can easily cross the BBB and facilitate the early detection of pathological conditions in the brain, such as glioma tumors (2) and Alzheimer’s disease (3), when these diseases are treatable. It is known that CAs that are based on a nanoparticle (NP) scaffold do not diffuse across the blood vessels and have a prolonged circulation half-life. Hence a lower concentration of the NPs, compared with the small molecule CAs, can be used for imaging the vasculature in animals. When NPs are coupled with a CA and a cell-surface binding ligand such as an apolipoprotein or an anti-transferrin receptor antibody, the NP-CA-ligand complex is able to cross cellular barriers, including the BBB, through the process of transcytosis (http://en.wikipedia.org/wiki/Transcytosis) (4). Investigators have shown that NPs made with human serum albumin (HSA; HSA-NPs) are non-toxic, biodegradable, and can be coupled with ligands such as transferrin (HSA-Tf-NP) to produce a complex that can cross the BBB (5). For a brief description of the nature and biological properties of transferrin, see Kolhatkar et al. (6). The use of transferrin for the targeted delivery of drugs in the brain is described by Dufes et al. (7). In another study, HSA-NPs loaded with gadolinium-labeled diethylenetriamine pentaacetic acid (Gd-DTPA; Gd-HSA-NPs) and coated with folic acid were shown to be able to cross the BBB and may be used with MRI for the noninvasive imaging of the brain in mice (8). In a continuing effort to develop NP-based CAs that can cross the BBB, Korkusuz et al. coupled the Gd-HSA-NPs with transferrin (Gd-HSA-Tf-NP) and studied the biodistribution of these NPs in normal mice (4). Gd-HSA-Tf-NP was also evaluated for use as a CA with MRI for imaging of the mouse brain.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Nanoparticles%20AND%20micad%5bbook%5d&cmd=DetailsSearch)

HSA nanoparticles in [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=HSA%20Nanoparticles&cmd=DetailsSearch)]

Protein (http://www.ncbi.nlm.nih.gov/protein/AAB22049.1) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/AH003008.1) sequences of human transferrin

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Transferrin&Search=Search) based on transferrin

Transferrin in Online Mendelian Inheritance in Man Database (OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=Transferrin))

Human transferrin in Gene Database (http://www.ncbi.nlm.nih.gov/gene/7018). Gene ID: 7018

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22811020%5Buid%5D&cmd=DetailsSearch)]

The synthesis of Gd-HSA-Tf-NPs has been detailed by Korkusuz et al. (4). Briefly, HAS-NPs were produced using the desolvation procedure (5), and Gd-DTPA was coupled to the NPs through N-(3-dimethylaminopropyl)-N-ethylcarbodiimide to obtain Gd-DTPA-HSA-NPs (Gd-HSA-NPs). A thiolated form of transferrin was conjugated to the Gd-HSA-NPs to produce Gd-HSA-Tf-NPs as described elsewhere (4). The number of transferrin molecules per NP was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gadolinium%20coated%20HSA%20transferrin%20nanoparticles%20in%20vitro%20studies&cmd=DetailsSearch)]

The average particle diameters of the Gd-HSA-NPs and the Gd-HSA-Tf-NPs were 190 ± 4 nm and 221 ± 5 nm, respectively, as determined with photon correlation spectroscopy, and the uniform size distribution of the NPs was confirmed with scanning electron microscopy (4). The particle content in the Gd-HSA-NP and the Gd-HSA-Tf-NP solutions were 6.5 ± 0.2 mg/mL and 7.1 ± 0.1 mg/mL, respectively. The Gd content of the Gd-DTPA-HSA-NPs and the Gd-DTPA-HSA-Tf-NPs were 45.6 ± 6.9 μg/mL and 73.3 ± 8.1 μg/mL, respectively, as determined with atomic absorption spectroscopy. The zeta potentials of the two preparations were −22.4 ± 7.4 mV and −19.9 ± 2.3 mV, respectively.

In vitro analysis of Gd-HSA-NPs and the Gd-HSA-Tf-NPs with MRI showed that the two NP preparations produced a contrast enhancement compared with the HSA-NPs and the HSA-Tf-NPs (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gadolinium%20coated%20HSA%20transferrin%20nanoparticles%20rodentia&cmd=DetailsSearch)]

The biodistributions of Gd-HSA-NPs and Gd-HSA-Tf-NPs were compared to that of Gd-DTPA in male mice (strain not reported) (4). The anesthetized animals (n = 5 mice/CA) were injected with 8 μmol/kg body weight (BW) equivalent Gd-DTPA of either Gd-HSA-NP or Gd-HSA-Tf-NP or 0.057 mmol/kg BW commercially available Gd-DTPA through the retrobulbar venous plexus. The rodents were placed in the coronal plane to acquire MRI images. Signal intensities were calculated from regions of interest drawn on the MRI images, and signal/noise ratios (SNR) were determined for the various tissues as described elsewhere (4) and are presented in Table 1. It was observed that Gd-HSA-Tf-NP generated a significantly higher (P < 0.05) signal in the mouse brain compared with either Gd-DTPA or Gd-HSA-NP. There was no significant difference (P > 0.05) between the SNRs of Gd-DTPA and Gd-HSA-NP. Although Gd-DTPA (P = 0.0221) and Gd-DTPA-Tf-NP (P = 0.0002) produced an enhanced signal in the skeletal muscles compared with the control mice, no such enhancement was observed with Gd-HSA-NP. Both Gd-HSA-NP (P < 0.0001) and Gd-HSA-Tf-NP (P < 0.0001) showed significantly higher contrast enhancement than Gd-DTPA in the blood, even though the Gd-DTPA content of the NPs was lower than the amount of Gd-DTPA injected by itself. In addition, the SNR of Gd-HSA-Tf-NP in the blood was significantly higher (P = 0.0113) than that of Gd-HSA-NP, indicating that coating Gd-HSA-NP with transferrin increased the contrast generated with these NPs in the blood. A significantly higher contrast was generated with Gd-HSA-Tf-NP in the heart muscle compared with either Gd-HSA-NP (P = 0.0138) or Gd-DTPA (P = 0.0057). The three NP CAs showed an increased SNR in the renal cortex and renal medulla compared to the SNR of the renal tissues from the control mice. This indicated that the CAs derived from Gd-DTPA and HSA-NP are excreted primarily through the renal route. Gd-DTPA, Gd-HSA-NP, and Gd-HSA-Tf-NP showed a higher contrast in the liver compared with the organ of the control animals. In addition, the signal in the liver was significantly higher with Gd-HSA-NP-Tf (P < 0.05) than with Gd-HSA-NP. This again indicated that modification of Gd-HSA-NP with transferrin increased the SNR of the modified NPs.

From these studies, the investigators concluded that Gd-HAS-Tf-NP was probably suitable for use as a CA with MRI to visualize the various parts of the brain in mice (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gadolinium%20coated%20HSA%20transferrin%20nanoparticles%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gadolinium%20coated%20HSA%20transferrin%20nanoparticles%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22811020%5Buid%5D&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Ichikawa H., Ishikawa M., Fukunaga M., Ishikawa K., Ishiyama H. (2010). Quantitative evaluation of blood-cerebrospinal fluid barrier permeability in the rat with experimental meningitis using magnetic resonance imaging. Brain Res.
2 Claes A., Gambarota G., Hamans B., van Tellingen O., Wesseling P., Maass C., Heerschap A., Leenders W. (2008). Magnetic resonance imaging-based detection of glial brain tumors in mice after antiangiogenic treatment. Int J Cancer.
3 Yang J., Wadghiri Y.Z., Hoang D.M., Tsui W., Sun Y., Chung E., Li Y., Wang A., de Leon M., Wisniewski T. (2011). Detection of amyloid plaques targeted by USPIO-Abeta1-42 in Alzheimer's disease transgenic mice using magnetic resonance microimaging. Neuroimage.
4 Korkusuz H., Ulbrich K., Welzel K., Koeberle V., Watcharin W., Bahr U., Chernikov V., Knobloch T., Petersen S., Huebner F., Ackermann H., Gelperina S., Kromen W., Hammerstingl R., Haupenthal J., Gruenwald F., Fiehler J., Zeuzem S., Kreuter J., Vogl T.J., Piiper A. (2013). Transferrin-coated gadolinium nanoparticles as MRI contrast agent. Mol Imaging Biol.
5 Ulbrich K., Hekmatara T., Herbert E., Kreuter J. (2009). Transferrin- and transferrin-receptor-antibody-modified nanoparticles enable drug delivery across the blood-brain barrier (BBB). Eur J Pharm Biopharm.
6 Kolhatkar R., Lote A., Khambati H. (2011). Active tumor targeting of nanomaterials using folic acid, transferrin and integrin receptors. Curr Drug Discov Technol.
7 Dufes C., Robaian M.A., Somani S. (2013). Transferrin and the transferrin receptor for the targeted delivery of therapeutic agents to the brain and cancer cells. Ther Deliv.
8 Korkusuz H., Ulbrich K., Bihrer V., Welzel K., Chernikov V., Knobloch T., Petersen S., Huebner F., Ackermann H., Gelperina S., Korkusuz Y., Kromen W., Hammerstingl R., Haupenthal J., Fiehler J., Zeuzem S., Kreuter J., Vogl T.J., Piiper A. (2012). Contrast enhancement of the brain by folate-conjugated gadolinium-diethylenetriaminepentaacetic acid-human serum albumin nanoparticles by magnetic resonance imaging. Mol Imaging.

Table 1:Signal/noise ratios of various tissues before and after the administration of Gd-DTPA, Gd-HSA-NP, or Gd-HSA-Tf-NP.

Tissues | No contrast | Gd-DTPA | Gd-HSA-NP | Gd-HSA-Tf-NP
Tissues | Signal/noise ratio (± standard deviation)
Brain | 12.1 ± 5.2 | 16.4 ± 1.2 | 17.0 ± 2.1 | 25.2 ± 1.6
Skeletal muscle | 11.3 ± 4.3 | 21.1 ± 5.1 | 14.9 ± 2.3 | 28.1 ± 5.1
Blood | 8.6 ± 2.8 | 17.7 ± 2.2 | 23.5 ± 3.6 | 30.1 ± 1.8
Heart muscle | 11.1 ± 4.1 | 19.4 ± 3.8 | 20.5 ± 5.0 | 29.5 ± 0.4
Kidney cortex | 14.4 ± 6.1 | 30.3 ± 4.2 | 24.0 ± 3.8 | 31.9 ± 8.1
Kidney medulla | 10.1 ± 3.8 | 28.8 ± 6.6 | 20.1 ± 3.2 | 26.7 ± 6.6
Liver | 11.0 ± 3.5 | 19.5 ± 2.5 | 17.1 ± 2.4 | 25.0 ± 1.9

For complete data, see Korkusuz et al. ( 4 ).